# ^68^Ga-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-Cpa-cyclo(D-Cys-amino-Phe-hydroorotic acid-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)-D-Tyr-NH_2_ (JR11)

Chemical name: | ^68^Ga-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-Cpa-cyclo(D-Cys-amino-Phe-hydroorotic acid-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)-D-Tyr-NH_2_ (JR11)
Abbreviated name: | ^68^Ga-DOTA-JR11
Synonym:
Agent category: | Peptide
Target: | Somatostatin receptor (SSTR2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=47117741), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=71979669) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6750) for more information about somatostatin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-JR11)]

Somatostatin (SST) is an inhibitor of the release of somatotropin, glucagon, insulin, gastrointestinal hormones, and other secretory proteins (1). SST is also known as the somatotropin release-inhibiting factor (SRIF). SST is a cyclic polypeptide with two biologically active isoforms, SRIF-14 and SRIF-28, of 14 and 28 amino acids, respectively. SRIF has a short plasma half-life of <3 min (2). SST receptors (SSTRs) (G-protein–coupled) have been found on a variety of neuroendocrine tumors and cells of the immune system, and five individual subtypes (SSTR1–SSTR5) have been identified and subsequently cloned from animal and human tissues (3, 4). SST also inhibits cell proliferation and promotes apoptosis through binding to specific cell-surface SSTRs (5).

^111^In-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-Octreotate (^111^In-DOTA-TATE) is an SST analog used in single-photon emission computed tomography (SPECT). Octreotate (D-Phe-c[Cys-D-Tyr-Trp-Lys-Thr-Cys]-Thr) is a cyclic peptide with eight amino acids. ^111^In-DOTA-TATE binds with high affinity to SSTR2, with little or no binding to other SSTRs. A large number of radiolabeled SST analogs have been reported using different radionuclides and different linkers. Most targeting SSTR peptides currently in use are SSTR2 agonists. Therefore, there is a need for SSTR2 antagonist radioligands because they tend to bind to both high and low affinity receptors (6). SSTR antagonists bind to a higher number of receptors than the agonists (7). Cpa-cyclo(D-Cys-amino-Phe-hydroorotic acid-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)-D-Tyr-NH_2_ (JR11) is a novel selective SSTR2 antagonist. Fani et al. (8) prepared ^68^Ga-DOTA-JR11 as a positron emission tomography (PET) imaging agent for SSTR2.

### Related Resource Links:

- Chapters in MICAD (somatostatin (http://www.ncbi.nlm.nih.gov/books?term=Somatostatin%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (somatostatin (http://www.ncbi.nlm.nih.gov/gene/6750), SSTR2 (http://www.ncbi.nlm.nih.gov/gene/6752))
- Articles in Online Mendelian Inheritance in Man (OMIM) (somatostatin (http://omim.org/entry/182450), SSTR2 (http://omim.org/entry/182452))
- Clinical trials (somatostatin receptor (http://www.clinicaltrials.gov/ct2/results?term=somatostatin+receptor))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-JR11+and+synthesis)]

DOTA-JR11 was synthesized via standard solid-phase peptide synthesis (8). DOTA was incorporated at the N-terminus of the peptide. DOTA-JR11 was purified with high-performance liquid chromatography. ^68^Ga was complexed to DOTA-JR11 by reaction of DOTA-JR11 with ^68^Ga in ammonium acetate buffer (pH 5.0) for 8 min at 95°C. ^68^Ga-DOTA-JR11 had a >95% radiochemical purity and specific activity of 80–100 MBq/nmol (2.2–2.7 mCi/nmol), with a labeling yield >97%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-JR11+and+in+vitro)]

Fani et al. (8) reported that NODAGA-JR11, ^nat^Ga-NODAGA-JR11, DOTA-JR11, and ^nat^Ga-DOTA-JR11 had 50% inhibition concentration (IC_50_) values of 4.1 ± 0.2, 1.2 ± 0.2, 0.72 ± 0.12, and 29 ± 3 nM, respectively, for human SSTR2 in competition with ^125^I-SRIF-28. The four JR11 conjugates (1,000 nM) exhibited little inhibition of the other SSTR subtypes. Immunofluorescence studies showed that the agonist [Tyr^3^]octreotide (10 nM) triggers receptor internalization, whereas ^nat^Ga-DOTA-JR11 at a much higher concentration (1,000 nM) does not stimulate receptor internalization in HEK-sst2 cells. This is another indication that JR11 is an antagonist. ^nat^Ga-DOTA-JR11 (1,000 nM) was able to inhibit receptor internalization induced by [Tyr^3^]octreotide.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-JR11+and+rodentia)]

Fani et al. (8) performed ex vivo biodistribution studies with 5–8 MBq (0.14–0.22 mCi) ^68^Ga-DOTA-JR11 in nude mice (n = 3–5/group) bearing HEK-sst2 xenografts at 1 h and 2 h after injection. The accumulation of radioactivity in the SSTR2 tumor was 23.8 ± 3.7% injected dose per gram (% ID/g) and 22.4 ± 7.6% ID/g at 1 h and 2 h, respectively. The kidney had the highest accumulation at 1 h (12.7% ID/g), followed by the adrenal (2.6% ID/g), bone (1.4% ID/g), and lung (1.0% ID/g). Low radioactivity levels (< 1% ID/g) were found in the other tissues and the SSTR2-positive tissues, such as the pancreas and stomach. The concentration in the blood was 0.6% ID/g at 1 h. The tumor/blood, tumor/liver, tumor/kidney, and tumor/muscle ratios at 1 h were 41.1, 50.7, 1.9, and 33.5, respectively. Co-injection with 1,500-fold excess DOTA-JR11 inhibited the SSTR2-positive tumor and adrenal radioactivity accumulation by 95% and 85% at 1 h, respectively. Little inhibition was observed in the SSTR2-negative tissues. At 1 h after injection, accumulation of ^68^Ga-DOTA-JR11 in the kidney was 20% higher and 22% lower in the tumor than that of ^68^Ga-NODAGA-JR11 in the same organs (P < 0.05). ^68^Ga-DOTA-JR11 exhibited 34% higher tumor and 144% higher kidney accumulation than the agonist ^68^Ga-DOTA-TATE (P < 0.05). ^68^Ga-DOTA-JR11 has a lower binding affinity (IC_50_ = 29 nM) to SSTR2 than ^68^Ga-DOTA-TATE (IC_50_ = 0.2 nM) yet exhibits higher binding to SSTR2-positive tumor. The higher number of binding sites for ^68^Ga-DOTA-JR11 (antagonist) versus^68^Ga-DOTA-TATE (agonist) more than compensates for the affinity difference.

Whole-body PET imaging visualized the SSTR2 tumor at 1 h and 2 h after injection of 5–8 MBq (0.14–0.22 mCi) ^68^Ga-DOTA-JR11 (8). The visualization was abrogated by co-injection of excess unlabeled DOTA-JR11.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-JR11+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-JR11+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DOTA-JR11+and+human)]

No publication is currently available.

## References

1 Weckbecker G., Lewis I., Albert R., Schmid H.A., Hoyer D., Bruns C. (2003). Opportunities in somatostatin research: biological, chemical and therapeutic aspects. Nat Rev Drug Discov.
2 Patel Y.C., Wheatley T. (1983). In vivo and in vitro plasma disappearance and metabolism of somatostatin-28 and somatostatin-14 in the rat. Endocrinology.
3 Corleto V.D., Nasoni S., Panzuto F., Cassetta S., Delle Fave G. (2004). Somatostatin receptor subtypes: basic pharmacology and tissue distribution. Dig Liver Dis.
4 Moller L.N., Stidsen C.E., Hartmann B., Holst J.J. (2003). Somatostatin receptors. Biochim Biophys Acta.
5 Barnett P. (2003). Somatostatin and somatostatin receptor physiology. Endocrine.
6 Reubi J.C., Schar J.C., Waser B., Wenger S., Heppeler A., Schmitt J.S., Macke H.R. (2000). Affinity profiles for human somatostatin receptor subtypes SST1-SST5 of somatostatin radiotracers selected for scintigraphic and radiotherapeutic use. Eur J Nucl Med.
7 Ginj M., Zhang H., Waser B., Cescato R., Wild D., Wang X., Erchegyi J., Rivier J., Macke H.R., Reubi J.C. (2006). Radiolabeled somatostatin receptor antagonists are preferable to agonists for in vivo peptide receptor targeting of tumors. Proc Natl Acad Sci U S A.
8 Fani M., Braun F., Waser B., Beetschen K., Cescato R., Erchegyi J., Rivier J.E., Weber W.A., Maecke H.R., Reubi J.C. (2012). Unexpected Sensitivity of sst2 Antagonists to N-Terminal Radiometal Modifications. J Nucl Med.